# ^18^F-(2S,4R)4-fluoroglutamine

Chemical name: | ^18^F-(2S,4R)4-fluoroglutamine
Abbreviated name: | [^18^F]4-FGln
Synonym: | [^18^F]-(2S,4R)4-fluoroglutamine
Agent Category: | Compound
Target: | Amino acid transporter
Target Category: | Transporter
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on above structure for information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=amino%20acid%20transporter&cmd=DetailsSearch)]

Increased growth and proliferation are the typical characteristic features of cancer cells, and to maintain these processes the cells have an increased demand for energy. Adenosine triphosphate is the main source of energy in normal cells, and it is produced through the tricarboxylic acid (TCA) cycle in the mitochondria. However, in cells with a malignant phenotype, the TCA is redirected to synthesize metabolic intermediates that can be used to produce fatty acids and amino acids (aa) that are required for the growth and survival of the tumor cells (1). To meet the energy requirements of cancerous tumors, the aerobic glycolytic pathway, which uses glucose to produce energy, is upregulated and serves as the major source of energy in the tumor cells (2). Therefore, [^18^F]-fluorodeoxyglucose ([^18^F]-FDG), an analog of glucose that is transported into and metabolized similarly to glucose in the cell (after phosphorylation to [^18^F]-FDG-6 phosphate it cannot be further metabolized by glycolysis and remains metabolically trapped within the cell), is often used to detect, stage, and monitor cancer therapy with positron emission tomography (PET) [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=fdg%20cancer&cmd=DetailsSearch)]. A major drawback of PET imaging with [^18^F]-FDG is that, in addition to tumor cells, normal cells in the brain, heart, brown adipose tissue, etc., also have high metabolic rates and utilize above-average amounts of glucose, which often leads to the generation of false positive results (2). Moreover, it is known that [^18^F]-FDG imaging cannot distinguish between infection, inflammation, and tumors (2).

There are indications that many tumors do not use the glycolytic pathway to produce energy and are consequently invisible to imaging with [^18^F]-FDG (1). Such tumors are believed to produce sufficient energy for survival by metabolizing other nutrients such as glutamine (for details, see Koglin et al. (3)), which has the highest concentration in the blood (up to ~1 mM) among all of the aa circulating in the blood and is metabolized through the glutaminolysis pathway (1). It is believed that tumors that cannot be visualized with PET using [^18^F]-FDG do not derive their energy through glycolysis and probably use the glutaminolysis pathway as an alternate source of energy. In a preliminary in vitro study with 9L (rat brain gliosarcoma cells) and SF188_Bcl-xL_ (of human glioblastoma origin) tumor cells that are addicted to glutamine (for details, see Wise and Thompson (4)), it was shown that both cell types had a higher uptake of ^18^F-labeled (2S,4R)4-fluoroglutamine ([^18^F]4-FGln; an analog of glutamine) than of [^3^H]-glutamine (5). It was also observed that the uptake of [^18^F]4-FGln by the 9L cells was inhibited by L-glutamine, which indicated that both the aa were taken up by the cells through a common transporter. On the basis of these observations, Lieberman et al. studied the biodistribution of [^18^F]4-FGln in normal mice and rats and in mice and rats bearing xenograft tumors (1). The ^18^F-labeled compound was also evaluated for the PET detection of tumors in mice and rats bearing these lesions.

### Related Resource Links

Amino acid transporter related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Amino+acid+transporter+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Amino acid transport across the plasma membrane [Reactome (http://pid.nci.nih.gov/search/pathway_landing.shtml?pathway_id=500341&pathway_name=Amino%20acid%20transport%20across%20the%20plasma%20membrane&source=Reactome%20Imported&what=graphic&jpg=on&ppage=1)]

Glycolysis pathway (http://pid.nci.nih.gov/search/pathway_landing.shtml?pathway_id=500677&pathway_name=Glycolysis&source=Reactome%20Imported&what=graphic&jpg=on&ppage=1)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The synthesis and ^18^F labeling of 4-FGln have been described by Lieberman et al. (1). The final labeled product had a non-decay-corrected radiochemical yield of 8.4 ± 3.4%, a radiochemical purity (RCP) of 98 ± 1%, and an optical purity of 91 ± 8% (results were derived from ten separate experiments). The specific activity of [^18^F]4-FGln was not reported.

The [^18^F]-FDG and L-[3,4-^3^H(N)]-glutamine ([^3^H]-Gln) for the in vitro cell uptake studies were purchased from commercial sources. The RCP and specific activity of [^18^F]-FDG were not mentioned. The RCP and specific activity of [^3^H]-Gln were >97% and1.11–2.22 TBq/mmol (~30–60 Ci/mmol), respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F%282S%2C4R%294-fluoroglutamine%20in%20vitro%20studies&cmd=DetailsSearch)]

The uptake of [^18^F]4-FGln was studied in 9L and SF188 cells (these cells have an amplified c-Myc oncogene that leads to glutamine addiction and increases uptake of the aa) as described elsewhere (1). Both cell lines showed a high uptake of [^18^F]4-FGln, and the 9L cells showed a linear increase in the incorporation of label up to a maximum of 15.7 ± 1.0% of the initial dose per 100 μg protein content (% ID/100 μg protein) at 120 min. The SF188 cells had a different kinetics of [^18^F]4-FGln uptake, and the maximum uptake of ~15% ID/100 μg protein was observed at 60 min, which decreased to ~10% ID/100 μg protein at 120 min.

In another study, the uptake of [^18^F]4-FGln, [^18^F]-FDG, and [^3^H]-Gln was studied in SF188_Bcl-xl_ cells (SF188_Bcl-xl_ cells transfected with the B-cell lymphoma extra large outer mitochondrial transmembrane anti-apoptotic protein), and these cells showed a higher incorporation of [^18^F]4-FGln from 30 min to 120 min than either [^18^F]-FDG or [^3^H]-Gln (1). From this study, the investigators concluded that the high uptake of [^18^F]4-FGln compared to the other two tracers was most likely due to upregulation of the c-Myc gene in these cells.

The incorporation of [^18^F]4-FGln into protein was measured at 30 min and 120 min in 9L and SF188 cells (1). For this study, [^3^H]-Gln was used as a reference ligand. Both tracers showed a similar profile of incorporation into the proteins. The incorporation of [^18^F]4-FGln and [^3^H]-Gln in the 9L cells was 29% and 72% at 30 min and 120 min, respectively, and with the SF188 cells the incorporation was 12% and 62%, respectively, at the two time points.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F%282S%2C4R%294-fluoroglutamine%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^18^F]4-FGln was investigated in normal Imprinting Control Region mice as described by Lieberman et al. (1). The animals (under anesthesia; n = 5 mice/time point) were injected with 925 KBq (25 μCi) [^18^F]4-FGln through the tail vein. The mice were euthanized at various time points ranging from 2 min to 240 min to remove the organs of interest and determine the amount of radioactivity accumulated in the different tissues. Data from this study were presented as percent of injected dose per gram tissue (% ID/g). From 2 min to 60 min postinjection (p.i.), the amount of label in the pancreas remained almost constant (~17.5% ID/g) before decreasing to 5.92 ± 0.87% ID/g at 240 min p.i. A similar trend was noted in the liver (6.92 ± 0.92% ID/g at 2 min p.i and 1.30 ± 0.18% ID/g at 240 min p.i.). The blood and lungs showed a gradual decrease in radioactivity from 6.19 ± 0.83% ID/g and 7.15 ± 0.76% ID/g, respectively, at 2 min p.i. to 0.48 ± 0.06% ID/g and 1.03 ± 0.15% ID/g, respectively, at 240 min p.i. A steady increase in radioactivity was observed in the bones (3.93 ± 0.37% ID/g at 2 min p.i and 19.4 ± 0.50% ID/g at 240 min p.i.), which the investigators suggested was probably due to the in vivo defluorination of [^18^F]4-FGln.

The in vivo biodistribution of [^18^F]4-FGln was also studied in Fischer 344 rats bearing 9L cell xenograft tumors (1). The animals (n = 6 animals/time point) were injected with 925 kBq (25 μCi) [^18^F]4-FGln as described above. The rats were euthanized at 30 min and 60 min p.i. to determine the amount of label accumulated in the tumors and various tissues. In general, the biodistribution of the tracer in the various organs of the rats was the same as that observed in the normal mice (described above). The uptake of radioactivity by the tumor was 1.03 ± 0.14% ID/g at 30 min p.i. and decreased slightly to 0.76 ± 0.21% ID/g at 60 min p.i. The tumor/blood and tumor/muscle ratios in the rats were 2.39 and 2.78, respectively, at 30 min p.i. and 2.37 and 2.00, respectively, at 60 min p.i.

Dynamic small-animal PET images of rats bearing 9L xenograft tumors and transgenic mice bearing M/tomND tumors (these are spontaneous lesions in animals that have an upregulated Myc gene) were acquired for up to 2 h after intravenous injection of [^18^F]4-FGln (1). From the images it was clear that the tumors could be visualized within 20 min after the injection, and the lesions remained visible for up to 2 h p.i. Ex vivo PET imaging of the organs and tumors obtained from the mice showed that the presence of radioactivity in the different tissues of the animals was consistent qualitatively with the biodistribution studies discussed above.

From these studies, the investigators concluded that [^18^F]4-FGln can probably be used for the detection of tumors in rodents (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F%282S%2C4R%294-fluoroglutamine%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F%282S%2C4R%294-fluoroglutamine%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22095958%5Buid%5D&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Lieberman B.P., Ploessl K., Wang L., Qu W., Zha Z., Wise D.R., Chodosh L.A., Belka G., Thompson C.B., Kung H.F. (2011). PET Imaging of Glutaminolysis in Tumors by 18F-(2S,4R)4-Fluoroglutamine. J Nucl Med.
2 Zhu A., Lee D., Shim H. (2011). Metabolic positron emission tomography imaging in cancer detection and therapy response. Semin Oncol.
3 Koglin N., Mueller A., Berndt M., Schmitt-Willich H., Toschi L., Stephens A.W., Gekeler V., Friebe M., Dinkelborg L.M. (2011). Specific PET imaging of xC- transporter activity using a (1)F-labeled glutamate derivative reveals a dominant pathway in tumor metabolism. Clin Cancer Res.
4 Wise D.R., Thompson C.B. (2010). Glutamine addiction: a new therapeutic target in cancer. Trends Biochem Sci.
5 Qu W., Zha Z., Ploessl K., Lieberman B.P., Zhu L., Wise D.R., Thompson C.B., Kung H.F. (2011). Synthesis of optically pure 4-fluoro-glutamines as potential metabolic imaging agents for tumors. J Am Chem Soc.